# ^11^C-Labeled GSK931145

Chemical name: | ^11^C-Labeled GSK931145
Abbreviated name: | [^11^C]GSK931145
Synonym:
Agent Category: | Compound
Target: | Glycine transporter 1 (GlyT-1)
Target Category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on structure for more information in PubChem. (http://www.ncbi.nlm.nih.gov/pccompound)

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=glycine%20transporter&cmd=DetailsSearch)]

The amino acid (aa) glycine acts as a neurotransmitter in the mammalian central nervous system (CNS) and modulates the neuroexcitatory activity of the N-methyl-D-aspartate (NMDA) receptor (NMDAR) through strychnine-insensitive glycine-binding sites located on the receptor (for details regarding the structure and function of NMDAR, see Paoletti et al. (1)). Impaired functioning of the NMDAR is believed to be responsible for the cognitive dysfunction (e.g., loss of reasoning, hallucinations, etc.) observed in individuals suffering from neuropsychiatric ailments, such as schizophrenia and related disorders; improving the activity of this receptor has been shown to be therapeutic (2, 3). Because glycine is an obligatory co-agonist of the NMDAR in the presence of D-serine, the glycine binding site on the receptor is considered to be a suitable therapeutic target for the treatment of schizophrenia (3). Specific sodium chloride–dependent transporters are responsible for transporting glycine into the CNS. However, rapid sequestration into the nerve terminals and surrounding glial cells by two high-affinity transporters, designated as GlyT-1 and GlyT-2, block the activity of glycine on the NMDAR in the synapse (3). GlyT-1 has been shown to maintain low levels of glycine at the synapse, which indicates that the aa controls neurotransmission through the NMDAR (3). It has been hypothesized that inhibition of GlyT-1 would increase glycine concentrations around the synapse, which would enhance the activity of the NMDAR. The use of GlyT-1 inhibitors could be a good approach to treat schizophrenia and other related cognitive afflictions (4). In addition, researchers are interested in using noninvasive imaging techniques to study any changes in the brains of individuals suffering from other neuropsychiatric disorders that may be associated with the GlyT-1. Therefore, several imaging agents, such as [^18^F]2,4-dichloro-N-((1-(propylsulphonyl)-4-(6-fluoropyridine-2-yl)piperidine-4-yl)methyl)benzamide ([^18^F]MK-6577 (5)) and [^11^C]GSK931145 (6-8), that can be used with positron emission tomography (PET) were developed. Among these, [^11^C]GSK931145 has been successfully evaluated for the in vivo visualization of GlyT-1 in pigs (8), non-human primates, and humans (6, 7).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amino+acid+transporter+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human GlyT-1 variant 3 protein and nucleotide sequences (http://www.genome.jp/dbget-bin/www_bget?refseq:NM_001024845) (RefSeq database)

GlyT-1 in Online Mendelian Inheritance in Man (OMIM) Database (http://omim.org/entry/601019)

GlyT-1 in Kyoto Encyclopedia of Genes and Genomics Database (http://www.genome.jp/dbget-bin/www_bget?hsa:6536)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=GlyT-1) related to GlyT-1

NMDAR in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nmdar)

What is schizophrenia? (http://www.nimh.nih.gov/health/publications/schizophrenia/what-is-schizophrenia.shtml) (National Institute of Mental Health web site)

Treatment (http://www.nimh.nih.gov/health/publications/schizophrenia/how-is-schizophrenia-treated.shtml) for schizophrenia (National Institute of Mental Health web site)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK931145%20synthesis&cmd=DetailsSearch)]

GSK931145 was obtained from a commercially supported Neuroscience Center of Excellence in Drug Discovery located in the United Kingdom, and the compound was labeled with ^11^C as described by Passchier et al. (8). The final labeled product had a radiochemical purity of >99% as determined with high-performance liquid chromatography (HPLC) and a specific activity of >39 GBq/μmol (>1.05 Ci/μmol). The radiochemical yield of the final labeled product was not reported. After purification, [^11^C]GSK931145 was formulated in normal saline and sterile filtered through a 0.22-μm filter into a vial for use in the different studies.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK931145%20in%20vitro&cmd=DetailsSearch)]

The pIC_50_ (-logIC_50_) values of GSK931145 for the GlyT-1 and GlyT-2 transporters were reported to be 8.4 and 4.6, respectively, indicating that the compound was highly selective for the GlyT-1 transporter (8). The pK_i_ (-logKi) values of GSK931145 in rat cortex was 8.97 (8). The partition coefficient (logD) of the drug was 2.53 (the logD of a drug should be <3 to cross the blood–brain barrier). The brain–blood area under the concentration-time curve ratio for GSK931145 was 1.9 (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK931145%20Rodentia&cmd=DetailsSearch)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK931145%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

The suitability of [^11^C]GSK931145 for the PET imaging of GlyT-1 in anesthetized pigs was evaluated by Passchier et al. (8). The animals (n = 6 pigs) were administered with 372 ± 84.4 MBq (8.83 ± 2.02 mCi) of the labeled compound through the femoral vein, and dynamic PET scans of the brain were acquired from 0 min to 90 min postinjection (p.i.). Blood samples were drawn from the animals at various time points varying from 5 min to 90 min p.i. to investigate metabolic degradation of the tracer. HPLC analysis of the plasma samples on a Phenomenex Sphereclone ODS column showed that ~75% of the labeled compound was metabolized by 60 min p.i. Qualitative analysis of the PET images showed that the radiolabeled probe could enter the brain, and the distribution of radioactivity at 40 min p.i. in the different areas of the organ was mesencephalon (~7.5% of injected dose per gram tissue (% ID/g)) > cerebellum (~6.0% ID/g) > cortex (~5% ID/g), which is consistent with the known distribution of GlyT-1 in the brain. In a blocking study, increasing concentrations of a nonradioactive GlyT-1 inhibitor (GSK565710; 1 μg/kg body weight (BW), 10 μg/kg BW, and 100 μg/kg BW)) were respectively administerd to one pig before the radiolabeled compound was injected into the animal, and PET images were acquired as before. Total volume of distribution estimates (V_T_) of the brain showed that there was a decrease in V_T_ for different regions of the organ with the increase in dose of GSK565710 (Table 1). This indicated that [^11^C]GSK931145 bound specifically to the GlyT-1 in these areas of the brain.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=20730499&cmd=DetailsSearch)]

The biodistribution of [^11^C]GSK931145 was studied in three baboons (Papio anubis) under anesthesia as described by Bullich et al. (6). The animals were given an intravenous injection (i.v.) of the tracer (81 ± 14 MBq (2.19 ± 0.4 mCi); specific activity 30 ± 5.5 GBq/μmol (0.273 ± 0.148 Ci/μmol)), and a series of whole-body PET images were acquired from the primates from 0 min to 80 min p.i. The residence time of radioactivity in the different organs (Table 2) was calculated from the area under the non-decay-corrected time-activity curves divided by the injected activity as described elsewhere (6).

From the data (Table 2), it was clear that the maximum residence time of radioactivity was the highest in the liver, followed by the heart, lungs, and brain. This indicated that the main route of clearance for this tracer was through the intestines.

In another study, four baboons were given an i.v. injection of [^11^C]GSK931145 (105 ± 44 MBq (2.83 ± 1.18 mCi)), and PET images were acquired from the animals for the next 120 min (7). From the images, it was apparent that there was rapid distribution of the tracer in the brain of the animals and that high amounts of radioactivity accumulated in the GlyT-1 rich areas of the organ (brain stem, thalamus, and cerebellum; range of accumulation at 20 min p.i. was ~14% injected dose per liter (% ID/L) to ~12% ID/L) compared with the cortex (has low expression of GlyT-1; accumulation at 20 min p.i. was ~7% ID/L). Prior administration of 0.5 mg/kg BW nonradioactive GSK931145 to the animals (n = 2 baboons) blocked the uptake of radioactivity from [^11^C]GSK931145 in the GlyT-1–rich areas, and a homogeneous distribution of the tracer was observed in the brain as detailed by Gunn et al. (7). HPLC analysis of the plasma obtained from the animals showed that, on average, ~30% of intact radioligand was present in the arterial plasma at 1 h p.i (7).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C-GSK931145%20Human%20Studies&cmd=DetailsSearch)]

The whole-body distribution of [^11^C]GSK931145 was investigated in eight healthy human volunteers (6). The individuals were given the tracer through an i.v. injection (average dose was 304.22 ± 112.87 MBq (8.21 ± 3.04 mCi), with an average specific activity of 21.57 ± 7.51 GBq/μmol (0.58 ± 0.20 Ci/μmol)). Whole-body PET scans were acquired from the individuals, and the residence time of radioactivity in the various organs was calculated as detailed by Bullich et al. (Table 3) (6).

The highest residence time of radioactivity was observed in the liver, followed by the lungs, heart, and brain, and this trend was similar to that observed with the baboons (6). Time-activity curves of the different organs showed there was a gradual loss of radioactivity from all the tissues over a period of 100 min.

In a second study, 13 healthy human volunteers were given an i.v. bolus of 429 ± 158 MBq (11.59 ± 4.3 mCi) [^11^C]GSK931145, and PET images of the brain were acquired from the individuals for the next 120 min (7). A rapid uptake of radioactivity was observed in the cerebellum, brain stem, and thalamus of the brain of the individuals (each region had ~1.7% ID/L at 40 min p.i.), which was similar to the observations made with the primate brain. In comparison, the cortex showed ~1% ID/L of radioactivity at this time point. When a blocking dose of GSK1018921 (200 mg; a GlyT-1 inhibitor) was administered to the individuals before i.v. injection of [^11^C]GSK931145, a homogeneous distribution of radioactivity was observed in the brain. The probe was metabolized during the entire duration of the study, and 60 ± 8% of the radioligand was reported to remain intact in the arterial plasma at 1 h p.i. as determined with HPLC (7).

From these studies, the investigators concluded that [^11^C]GSK931145 can be used for the imaging of GlyT-1 with PET in pigs (8), primates, and humans (7).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Paoletti P. (2011). Molecular basis of NMDA receptor functional diversity. Eur J Neurosci.
2 Shim S.S., Hammonds M.D., Kee B.S. (2008). Potentiation of the NMDA receptor in the treatment of schizophrenia: focused on the glycine site. Eur Arch Psychiatry Clin Neurosci.
3 Hashimoto K. (2011). Glycine transporter-1: a new potential therapeutic target for schizophrenia. Curr Pharm Des.
4 Wolkenberg S.E., Sur C. (2010). Recent progress in the discovery of non-sarcosine based GlyT1 inhibitors. Curr Top Med Chem.
5 Hamill T.G., Eng W., Jennings A., Lewis R., Thomas S., Wood S., Street L., Wisnoski D., Wolkenberg S., Lindsley C., Sanabria-Bohorquez S.M., Patel S., Riffel K., Ryan C., Cook J., Sur C., Burns H.D., Hargreaves R. (2011). The synthesis and preclinical evaluation in rhesus monkey of [(1)F]MK-6577 and [(1)(1)C]CMPyPB glycine transporter 1 positron emission tomography radiotracers. Synapse.
6 Bullich S., Slifstein M., Passchier J., Murthy N.V., Kegeles L.S., Kim J.H., Xu X., Gunn R.N., Herance R., Gispert J.D., Gutierrez A., Farre M., Laruelle M., Catafau A.M. (2011). Biodistribution and radiation dosimetry of the glycine transporter-1 ligand 11C-GSK931145 determined from primate and human whole-body PET. Mol Imaging Biol.
7 Gunn R.N., Murthy V., Catafau A.M., Searle G., Bullich S., Slifstein M., Ouellet D., Zamuner S., Herance R., Salinas C., Pardo-Lozano R., Rabiner E.A., Farre M., Laruelle M. (2011). Translational characterization of [(11) C]GSK931145, a PET ligand for the glycine transporter type 1. Synapse.
8 Passchier J., Gentile G., Porter R., Herdon H., Salinas C., Jakobsen S., Audrain H., Laruelle M., Gunn R.N. (2010). Identification and evaluation of [11C]GSK931145 as a novel ligand for imaging the type 1 glycine transporter with positron emission tomography. Synapse.

Table 1: Total volume of distribution estimates (V_T_) for [^11^C]GSK931145 in different regions of the pig brain after the animal was given blocking doses of unlabeled GSK565710.

Region of brain | Baseline | Dose of unlabeled GSK565710 (μg/kg body weight)
Region of brain | Baseline | 1 | 10 | 100
Region of brain | Baseline | (V _ T _ ; (ml/cm ^ 3 ^ )
Mesencephalon | 11.60 | 9.15 | 6.32 | 3.00
Cerebellum | 6.93 | 5.56 | 4.45 | 2.42
Cortex | 5.08 | 4.35 | 3.40 | 2.20

For complete data, see Passchier et al. (8).

Table 2: Residence time of radioactivity from [^11^C]GSK931145 in various organs of baboons (n = 3 animals)

Organ | Residence time (h)
Liver | 0.087 ± 0.011
Lungs | 0.054 ± 0.013
Heart | 0.056 (n = 1)
Brain | 0.021 ± 0.003
Kidneys | 0.006 ± 0.001
Remainder of body | 0.297 ± 0.013

For complete data see Bullich et al. (6)

Table 3: Residence time of radioactivity from [^11^C]GSK931145 in various organs of humans (n = 8 individuals).

Organ | Residence time (h)
Liver | 0.053 ± 0.014
Lungs | 0.024 ± 0.006
Heart | 0.014 ± 0.003
Brain | 0.010 ± 0.003
Kidneys | 0.003 ± 0.001
Remainder of body | 0.326 ± 0.032

For complete data, see Bullich et al (6).